# 5-(2E,4E)-5-(6-hydroxy-4-oxo-2-thioxo-1,2,3,4-tetrahydroxy-5 pyrimidinyl)-2,4-pentadienylidene-2-thioxodihydro-4,6(1H,5H)-pyrimidinedione

Chemical name: | 5-(2E,4E)-5-(6-hydroxy-4-oxo-2-thioxo-1,2,3,4-tetrahydroxy-5 pyrimidinyl)-2,4-pentadienylidene-2-thioxodihydro-4,6(1H,5H)-pyrimidinedione
Abbreviated name: | THK-265
Synonym:
Agent category: | Compound
Target: | Amyloid-beta (Aβ) peptide
Target category: | Acceptor
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal: | THK-265
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=THK-256)]

Alzheimer's disease (AD) is a form of dementia with gradual memory loss and a progressive decline in mental functions over time (1, 2). It is characterized pathologically by neuronal loss, extracellular senile plaques (aggregates of amyloid-beta (Aβ) peptides consisting of 40–42 amino acids formed as the proteolytic cleavage of Aβ protein precursor (AβPP)), and intracellular neurofibrillary tangles (filaments of microtubule-binding hyper-phosphorylated protein tau) in the brain, especially in the hippocampus and associative regions of the cortex (3, 4). Aβ peptides and tau protein are implicated as the main causes of neuronal degeneration and cell death (5, 6). Early diagnosis of AD is important for treatment consideration and disease management (7). Various Aβ imaging agents have been developed for magnetic resonance imaging (MRI), single-photon emission computed tomography (SPECT), and positron emission tomography (PET) (8-13). The binding of different derivatives of Congo red, thioflavin, stilbene, and aminonaphthalene has been studied in human postmortem brain tissue and in transgenic mice. 2-(1-(6-[(2-[^18^F]fluoroethyl)(methyl)amino]-2-naphthyl)ethylidene)malono nitrile ([^18^F]FDDNP) has been studied in humans, showing more binding in the brains of patients with AD than in those of healthy people (14). However, [^18^F]FDDNP showed low signal/noise ratios for PET imaging because it is highly lipophilic. N-methyl-[^11^C]-2-(4'-methylaminophenyl)-6-hydroxybenzothiasole, a Aβ binding compound based on a series of neutral thioflavin-T derivatives (15), was radiolabeled with the positron-emitting radionuclide ^11^C ([^11^C]6-OH-BTA-1 or [^11^C]PIB). [^11^C]6-OH-BTA-1 was found to be a promising imaging agent for senile plaques in the brain (16). Zhang et al. (17) reported the development of a series of fluorinated polyethylene glycol (PEG) units (n = 2–5) for PET imaging of Aβ plaques in the brain. Two of them, [^18^F]BAY94-9172 (http://www.ncbi.nlm.nih.gov/books/NBK23203/) ([^18^F]AV-1) (18) and ([^18^F]AV-45 (http://www.ncbi.nlm.nih.gov/books/NBK32300/), also known as [^18^F]Florbetapir) (19), have been evaluated in clinical trials. [^18^F]Florbetapir is approved for estimation of brain amyloid plaque content in patients with cognitive decline by the United States Food and Drug Administration (US FDA (http://www.fda.gov/NewsEvents/Newsroom/PressAnnouncements/ucm299678.htm?utm_campaign=Google2&utm_source=fdaSearch&utm_medium=website&utm_term=amyloid&utm_content=3)).

Optical imaging is increasingly being used to monitor biological functions of specific targets in vitro and in vivo to provide real-time imaging (20-22). Small near-infrared (NIR) fluorescence probes (emission wavelength, 650–900 nm) exhibit a reduction of the natural background fluorescence interference of biomolecules, providing a high contrast between target and background tissues in small animals. A number of optical probes for the detection of Aβ plaques are available, such as Congo red, thioflavin, CRANAD-2, and AOI987 (23, 24). Okamura et al. (25) evaluated 5-(2E,4E)-5-(6-hydroxy-4-oxo-2-thioxo-1,2,3,4-tetrahydroxy-5 pyrimidinyl)-2,4-pentadienylidene-2-thioxodihydro-4,6(1H,5H)-pyrimidinedione (THK-265) as a NIR fluorescence imaging probe for in vivo imaging of Aβ in an animal model of AD.

### Related Resource Links:

- Chapters in MICAD (amyloid (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=amyloid+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (amyloid (http://www.ncbi.nlm.nih.gov/gene/351))
- Articles in Online Mendelian Inheritance in Man (OMIM) (amyloid (http://www.ncbi.nlm.nih.gov/omim/?term=Amyloid))
- Clinical trials (amyloid (http://www.clinicaltrials.gov/ct2/results?term=Amyloid))
- Drug information in FDA (amyloid inhibitors (http://google2.fda.gov/search?q=Amyloid+inhibitor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=16&y=16))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=THK-256%20and%20synthesis)]

THK-265 is commercially available (Organica, Wolfen, Germany) (25). THK-265 displayed the following fluorescent properties in methanol: one single absorption maximum at 627 nm, one single emission maximum at 644 nm, a high absorption coefficient of 96,198 M^–1^cm^–1^, and a high quantum yield of 38.5%. Similar maximum excitation and emission wavelengths were observed in human serum and potassium phosphate buffer (pH, 7.4). THK-265 exhibited a log P value of 1.8 ± 0.8 (moderate lipophilicity).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=THK-256%20and%20in%20vitro)]

Differential fluorescence spectroscopy performed by Okamura et al. (25) showed that the magnitude of the fluorescence increase was dependent on the concentration of THK-265 (3–1,000 nM) in the presence of aggregated Aβ peptides (5 µM). The K_d_ value for THK-265 was estimated to be 97 ± 5 nM, which was lower than that of AOI987 (200 nM). THK-265 staining of amyloid plaques was observed in postmortem brain tissues of the brain (the surface region of frontal cortex) of one AD male patient (age 69 years). THK-265 staining pattern colocalized with Aβ immunostaining. THK-265 also stained neurofibrillary tangles.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=THK-256%20and%20rodentia)]

The blood–brain barrier (BBB) penetration of THK-265 was assessed ex vivo using 7-week-old wild-type (Wt) male mice (n = 3–4/group) after intravenous injection of 1 mg/kg THK-265 (25). Brain accumulation levels of THK-265 were 0.04% injected dose per gram (ID/g) at 2 min and 0.0065% ID/g at 30 min as measured with high-performance liquid chromatography. Ex vivo NIR fluorescence imaging showed that THK-265 entered the brain rapidly (6.2 × 10^7^ p/s/cm^2^/sr) at 2 min and was then gradually eliminated from the brain, with 2.4 × 10^7^ p/s/cm^2^/sr and 2.1 × 10^7^ p/s/cm^2^/sr at 60 min and 120 min, respectively. No acute toxicity of THK-265 at 10 mg/kg in normal mice was observed up to 7 days after injection.

In vivo NIR fluorescence imaging of Aβ using THK-265 (1 mg/kg) was performed in 19-month-old (19M) and 32-month-old (32M) AβPP transgenic (Tg) and age-matched Wt female mice (n = 3/group) at 0, 3, 30, 64, and 118 min after injection (25). THK-265 entered rapidly into the brains and was consistently higher in Tg mice than in Wt mice. Fluorescence intensity levels at 3 min after injection were 3.8, 2.6, 1.8, and 1.7 × 10^8^ p/s/cm^2^/sr for 32M Tg, 19M Tg, 32M Wt, and 19M Wt mice, respectively. Additional studies were performed in 27M Tg and 27M Wt mice with THK-265, AOI987, and ICG. Both THK-265 and AOI987 showed higher fluorescence signals in Tg mice than in Wt mice, whereas ICG showed similar fluorescence signals in both types of mice. The brain/neck ratios at 113 min after injection were 1.2, 1.2, 1.2, 1.6, 1.3, and 2.2 for ICG/Wt, ICG/Tg, AOI987/Wt, AOI987/Tg, THK-265/Wt, and THK-265/Tg, respectively. THK-265 displayed similar brain/neck ratios with AOI987 and ICG in the Wt mice but significantly higher ratios than AOI987 and ICG in the Tg mice (P < 0.05). There was a significant correlation (r = 0.943, P < 0.017) of THK-265 brain/neck ratios with the number of amyloid plaques in Tg mice.

Schmidt et al. (26) performed in vivo NIR fluorescence imaging of Aβ using THK-265 (1 mg/kg) using younger Tg and Wt mice (75, 100, and 200 d) (n = 5/group) at 10, 20, 30, 60, and 90 min after injection. There was an increase of signal in the Tg mice correlating with age, whereas little change in signal was observed in Wt mice versus baseline background. Quantitative analysis of fluorescence signals in the brain at 30 min after injection showed that Tg (75 d), Tg (100 d), and Tg (200 d) mice exhibited 20%, 80%, and 140% increase in signal compared with the age-matched Wt mice. Histological analysis showed that there was co-localization of THK-265 staining with amyloid plaques and an increasing number of amyloid plaques with stronger fluorescence signal.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=THK-256%20and%20%28dog%20or%20pig%20or%20cat%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=THK-256%20and%20primate%20not%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=THK-256%20and%20humans)]

No publication is currently available.

## References

1 Forstl H., Kurz A. (1999). Clinical features of Alzheimer's disease. Eur Arch Psychiatry Clin Neurosci.
2 Heininger K. (2000). A unifying hypothesis of Alzheimer's disease. IV. Causation and sequence of events. Rev Neurosci.
3 Mirra S.S., Heyman A., McKeel D., Sumi S.M., Crain B.J., Brownlee L.M., Vogel F.S., Hughes J.P., van Belle G., Berg L. (1991). The Consortium to Establish a Registry for Alzheimer's Disease (CERAD). Part II. Standardization of the neuropathologic assessment of Alzheimer's disease. Neurology.
4 Hardy J.A., Higgins G.A. (1992). Alzheimer's disease: the amyloid cascade hypothesis. Science.
5 Hardy J. (2003). The relationship between amyloid and tau. J Mol Neurosci.
6 Brandt R., Hundelt M., Shahani N. (2005). Tau alteration and neuronal degeneration in tauopathies: mechanisms and models. Biochim Biophys Acta.
7 de Leon M.J., DeSanti S., Zinkowski R., Mehta P.D., Pratico D., Segal S., Clark C., Kerkman D., DeBernardis J., Li J., Lair L., Reisberg B., Tsui W., Rusinek H. (2004). MRI and CSF studies in the early diagnosis of Alzheimer's disease. J Intern Med.
8 Bacskai B.J., Klunk W.E., Mathis C.A., Hyman B.T. (2002). Imaging amyloid-beta deposits in vivo. J Cereb Blood Flow Metab.
9 Nordberg A. (2004). PET imaging of amyloid in Alzheimer's disease. Lancet Neurol.
10 Mathis C.A., Wang Y., Klunk W.E. (2004). Imaging beta-amyloid plaques and neurofibrillary tangles in the aging human brain. Curr Pharm Des.
11 Klunk W.E., Engler H., Nordberg A., Bacskai B.J., Wang Y., Price J.C., Bergstrom M., Hyman B.T., Langstrom B., Mathis C.A. (2003). Imaging the pathology of Alzheimer's disease: amyloid-imaging with positron emission tomography. Neuroimaging Clin N Am.
12 Wang Y., Klunk W.E., Debnath M.L., Huang G.F., Holt D.P., Shao L., Mathis C.A. (2004). Development of a PET/SPECT agent for amyloid imaging in Alzheimer's disease. J Mol Neurosci.
13 Kung M.P., Hou C., Zhuang Z.P., Skovronsky D., Kung H.F. (2004). Binding of two potential imaging agents targeting amyloid plaques in postmortem brain tissues of patients with Alzheimer's disease. Brain Res.
14 Shoghi-Jadid K., Small G.W., Agdeppa E.D., Kepe V., Ercoli L.M., Siddarth P., Read S., Satyamurthy N., Petric A., Huang S.C., Barrio J.R. (2002). Localization of neurofibrillary tangles and beta-amyloid plaques in the brains of living patients with Alzheimer disease. Am J Geriatr Psychiatry.
15 Bacskai B.J., Hickey G.A., Skoch J., Kajdasz S.T., Wang Y., Huang G.F., Mathis C.A., Klunk W.E., Hyman B.T. (2003). Four-dimensional multiphoton imaging of brain entry, amyloid binding, and clearance of an amyloid-beta ligand in transgenic mice. Proc Natl Acad Sci U S A.
16 Klunk W.E., Engler H., Nordberg A., Wang Y., Blomqvist G., Holt D.P., Bergstrom M., Savitcheva I., Huang G.F., Estrada S., Ausen B., Debnath M.L., Barletta J., Price J.C., Sandell J., Lopresti B.J., Wall A., Koivisto P., Antoni G., Mathis C.A., Langstrom B. (2004). Imaging brain amyloid in Alzheimer's disease with Pittsburgh Compound-B. Ann Neurol.
17 Zhang W., Oya S., Kung M.P., Hou C., Maier D.L., Kung H.F. (2005). F-18 Polyethyleneglycol stilbenes as PET imaging agents targeting Abeta aggregates in the brain. Nucl Med Biol.
18 O'Keefe G.J., Saunder T.H., Ng S., Ackerman U., Tochon-Danguy H.J., Chan J.G., Gong S., Dyrks T., Lindemann S., Holl G., Dinkelborg L., Villemagne V., Rowe C.C. (2009). Radiation Dosimetry of {beta}-Amyloid Tracers 11C-PiB and 18F-BAY94-9172. J Nucl Med.
19 Choi S.R., Golding G., Zhuang Z., Zhang W., Lim N., Hefti F., Benedum T.E., Kilbourn M.R., Skovronsky D., Kung H.F. (2009). Preclinical properties of 18F-AV-45: a PET agent for Abeta plaques in the brain. J Nucl Med.
20 Frangioni J.V. (2008). New technologies for human cancer imaging. J Clin Oncol.
21 Pan D., Caruthers S.D., Chen J., Winter P.M., SenPan A., Schmieder A.H., Wickline S.A., Lanza G.M. (2010). Nanomedicine strategies for molecular targets with MRI and optical imaging. Future Med Chem.
22 Schaafsma B.E., Mieog J.S., Hutteman M., van der Vorst J.R., Kuppen P.J., Lowik C.W., Frangioni J.V., van de Velde C.J., Vahrmeijer A.L. (2011). The clinical use of indocyanine green as a near-infrared fluorescent contrast agent for image-guided oncologic surgery. J Surg Oncol.
23 Hintersteiner M., Enz A., Frey P., Jaton A.L., Kinzy W., Kneuer R., Neumann U., Rudin M., Staufenbiel M., Stoeckli M., Wiederhold K.H., Gremlich H.U. (2005). In vivo detection of amyloid-beta deposits by near-infrared imaging using an oxazine-derivative probe. Nat Biotechnol.
24 Ran C., Xu X., Raymond S.B., Ferrara B.J., Neal K., Bacskai B.J., Medarova Z., Moore A. (2009). Design, synthesis, and testing of difluoroboron-derivatized curcumins as near-infrared probes for in vivo detection of amyloid-beta deposits. J Am Chem Soc.
25 Okamura N., Mori M., Furumoto S., Yoshikawa T., Harada R., Ito S., Fujikawa Y., Arai H., Yanai K., Kudo Y. (2011). In vivo detection of amyloid plaques in the mouse brain using the near-infrared fluorescence probe THK-265. J Alzheimers Dis.
26 Schmidt A., Pahnke J. (2012). Efficient Near-Infrared In Vivo Imaging of Amyoid-beta Deposits in Alzheimer's Disease Mouse Models. J Alzheimers Dis.